# ^99m^Tc-Labeled rituximab, a chimeric murine/human anti-CD20 monoclonal antibody

Chemical name: | ^99m^Tc-Labeled rituximab, a chimeric murine/human anti-CD20 monoclonal antibody
Abbreviated name: | [^99m^Tc]Rituximab
Synonym: | MabThera®; Rituxan®
Agent Category: | Antibody
Target: | Cell differentiation antigen 20 (CD20)
Target Category: | Antigen
Method of detection: | Single-photon emission tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Humans | Structure not available in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=rituximab&cmd=DetailsSearch)]

Rituximab (http://dailymed.nlm.nih.gov/dailymed/lookup.cfm?setid=b172773b-3905-4a1c-ad95-bab4b6126563) is a chimeric murine/human monoclonal antibody (mAb) that targets the CD20 antigen (also known as membrane-spanning 4-domains, subfamily A, member 1; or MS4A1), which is expressed on 95% of the transformed B-cells that participate in the pathogenesis of non-Hodgkin lymphomas (http://cancer.gov/cancertopics/types/non-hodgkin) (NHL; diffused large-B cell, low-grade, or the follicular types), a hematological malignancy, and autoimmune diseases such as rheumatoid arthritis (http://www.nlm.nih.gov/medlineplus/rheumatoidarthritis.html) (RA), granulomatosis with polyangiitis (http://www.rheumatology.org/practice/clinical/patients/diseases_and_conditions/wegeners.asp) (Wegener's granulomatosis), and microscopic polyangiitis (http://rarediseases.info.nih.gov/GARD/Condition/3652/Microscopic_polyangiitis.aspx). The CD20 antigen is not expressed on any other hematopoietic cells and is not shed for circulation into the plasma or internalized by the cells (1). Therefore, the CD20 antigen is considered to be an excellent target for the treatment of the various B-lymphocyte, cell-based diseases such as those mentioned above. The United States Food and Drug Administration has approved the use of rituximab for the treatment of NHL and the other diseases mentioned above. The exact mechanism of action of rituximab has been discussed by Maloney (2). Although much is known about the pathogenesis of the different forms of NHL at the molecular level, the prognosis for an individual suffering from this disease is based on the morphological and histological information obtained with invasive methods used on the patients (3). As an alternative to the invasive methods, noninvasive procedures, such as imaging with radiolabeled agents using single-photon emission computed tomography (SPECT) or positron emission tomography, are attractive options to screen for patients who can benefit the most from an anti-cancer treatment, and the same imaging technique(s) can be used to monitor and assess the efficacy of a treatment (4).

Rituximab was labeled with ^99m^Tc ([^99m^Tc]rituximab) and used with SPECT for the imaging of NHL (1) and several inflammatory autoimmune diseases such as RA, Behcet’s disease (http://www.mayoclinic.com/health/behcets-disease/DS00822), sarcoidosis (http://www.lung.org/lung-disease/sarcoidosis/?gclid=CJWYisCI2bICFc2d4AodzRsApQ), and others, in humans (5).

### Related Resource Links

Related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=Rituximab+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Human CD20 protein (http://www.ncbi.nlm.nih.gov/protein/NP_068769.2) and mRNA (http://www.ncbi.nlm.nih.gov/nuccore/NM_152866.2) (membrane spanning 4-domains, subfamily, member 1 (MS4A1) transcript variant 1) sequences

Human CD20 in Gene database (http://www.ncbi.nlm.nih.gov/gene/931); Gene ID: 931

Information on human CD20 in Online Mendelian Inheritence in Man database (OMIM (http://omim.org/entry/112210))

Clinical trials (http://clinicaltrials.gov/ct2/results?term=CD20&Search=Search) regarding CD20

Rituximab-related clinical trials (http://clinicaltrials.gov/ct2/results?term=Rituximab&Search=Search)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc-rituximab%20synthesis&cmd=DetailsSearch)]

Rituximab was purified from a commercial formulation of the mAb and labeled with ^99m^Tc using a photo-activation procedure as described by Stopar et al. (6). The radiolabeling yield of the reaction was >95% as determined with thin-layer chromatography (TLC) and size-exclusion high performance liquid chromatography. The radiochemical purity (RCP) and specific activity of [^99m^Tc]rituximab were not reported.

In another study, [^99m^Tc]rituximab was prepared with a direct labeling method for use in humans (5). The labeling efficiency of the reaction was reported to be >98%, and the preparation contained <2% colloids as determined with instant TLC. The labeled mAb was used in humans without further purification. The specific activity of [^99m^Tc]rituximab was 3.5–3.7 GBq/6.66 nmol (94.5–100 mCi/6.66 nmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc-rituximab%20in%20vitro&cmd=DetailsSearch)]

After storage at room temperature for 24 h, the RCP of [^99m^Tc]rituximab was reported to be 95%–97.2% as determined with TLC (6). The tracer had an RCP of 89% after storage in serum (source not mentioned) for 24 h at 37°C (6).

The [^99m^Tc]rituximab preparation was reported to have an immunoreactive fraction of 93.5% as determined in a binding assay with Ramos cells (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-1596&Template=cellBiology) (6). The dissociation constant of [^99m^Tc]rituximab was 2.9 nM, and the cells had a maximum binding capacity of 0.98 pmol labeled mAb per 10^6^ cells, indicating that ~6 × 10^5^ molecules of the tracer could bind to each cell (6). The binding of [^99m^Tc]rituximab to Ramos cells increased from 4.7% of the total applied radioactivity to 23.9% at 4 h at 37^o^ C and approximately 5% of the total added radioactivity was internalized by the cells (incubated with cell growth medium) (6). By comparison, the binding on the control cells was only 12.6% of the total added tracer at 4 h with almost no internalization (control cells were incubated with [^99m^Tc]rituximab on ice for the same duration as the Ramos cells, in phosphate-buffered saline (pH 7.0) containing 1% human serum albumin) (6).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20rodentia)]

No publication is currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc-rituximab%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc-rituximab%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc-rituximab%20Human%20Studies&cmd=DetailsSearch)]

The use of [^99m^Tc]rituximab was evaluated to assess the expression of CD20 in NHL patients (n = 10 individuals); nine patients had CD20^+^ B-cell NHL; one patient had CD20^–^ NHL. Among the ten patients, five individuals had follicular NHL and diffuse large cell B-lymphoma, respectively (1). The patients were intravenously administered 500–600 MBq (18.5–22.2 mCi) [^99m^Tc]rituximab, and whole-body scintigraphic images were acquired from the individuals at 6 h and 20 h postinjection (p.i.). To study early biodistribution of the tracer, additional images were acquired from three patients at 1 h and 3–4 h p.i. At 1 h p.i. and 3 h p.i., the images showed that the radioactivity was present mainly in the blood and the liver of the patients, but at 3 h p.i. some accumulation was also visible in the kidneys and the spleen (1). At 3 h p.i., one patient with a splenic lymphoma showed high uptake of the tracer in the spleen. In three patients, the tumors were clearly visible at 20 h p.i. compared with the earlier time point. From this study, the investigators concluded that [^99m^Tc]rituximab was probably a suitable imaging agent to assess the expression of CD20 and to visualize spread of the B-cell NHL disease in humans (1).

In another study, the use of [^99m^Tc]rituximab was assessed for the imaging of B-lymphocyte infiltration in the affected tissues of patients with chronic inflammatory autoimmune disease (n = 20 individuals) (5). The patients were given an intravenous injection of 350–370 MBq (9.5–10 mCi; 600 pmol) [^99m^Tc]rituximab, and whole-body SPECT images were acquired from the individuals at 6 h p.i. and 20 h p.i. The label was observed to accumulate rapidly in the spleen, and the radioactivity was excreted primarily through the urinary route in all the patients. At 6 h p.i., the inflamed joints were clearly visible in the patients with RA; the salivary and lacrimal glands showed variable uptake of radioactivity in patients with Sjögren’s syndrome; moderate lung uptake was evident in a patient with sarcoidosis; a patient with Behçet’s disease showed increased accumulation of radioactivity in the oral mucosa; moderately high uptake of label was evident in the neck cartilage of a patient with polychondritis; and a moderate to high accumulation of the tracer was observed in the skin of dermatopolymyositis patients (5). From this study, the investigators concluded that [^99m^Tc]rituximab can probably be used to assess the infiltration of B lymphocyte in the affected organs of patients suffering from the different types of autoimmune diseases (5).

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Gmeiner Stopar T., Fettich J., Zver S., Mlinaric-Rascan I., Hojker S., Socan A., Peitl P.K., Mather S. (2008). 99mTc-labelled rituximab, a new non-Hodgkin's lymphoma imaging agent: first clinical experience. Nucl Med Commun.
2 Maloney D.G. (2012). Anti-CD20 antibody therapy for B-cell lymphomas. N Engl J Med.
3 Natarajan A., Gowrishankar G., Nielsen C.H., Wang S., Iagaru A., Goris M.L., Gambhir S.S. (2012). Positron Emission Tomography of (64)Cu-DOTA-Rituximab in a Transgenic Mouse Model Expressing Human CD20 for Clinical Translation to Image NHL. Mol Imaging Biol.
4 Willmann J.K., van Bruggen N., Dinkelborg L.M., Gambhir S.S. (2008). Molecular imaging in drug development. Nat Rev Drug Discov.
5 Malviya G., Anzola K.L., Podesta E., Lagana B., Del Mastro C., Dierckx R.A., Scopinaro F., Signore A. (2012). (99m)Tc-labeled Rituximab for Imaging B Lymphocyte Infiltration in Inflammatory Autoimmune Disease Patients. Mol Imaging Biol.
6 Stopar T.G., Mlinaric-Rascan I., Fettich J., Hojker S., Mather S.J. (2006). (99m)Tc-rituximab radiolabelled by photo-activation: a new non-Hodgkin's lymphoma imaging agent. Eur J Nucl Med Mol Imaging.